# ^124^I/^64^Cu-Labeled anti-CD20 minibody

Chemical name: | [^124^I/^64^Cu]Anti-CD20 minibody
Abbreviated name: | [^124^I/^64^Cu]Anti-CD20 ScFv-C_H_3 dimer
Synonym:
Agent Category: | Antibody
Target: | CD-20
Target Category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^124^I/^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/P11836.1?ordinalpos=1&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_021950.3?ordinalpos=1&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=human+CD20) for information regarding human CD20.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti-CD20+minibody)]

The B cell differentiation antigen (CD20) is a transmembrane, non-glycosylated, hydrophobic protein that is characteristically expressed in more than 90% of non-Hodgkin lymphoma (NHL) tumors. Although the exact cellular functions of CD20 are not known, it is believed to play a role in B cell growth, activation, and maintenance of cellular calcium homeostasis (1). Because of its specific presence in the NHL tumor cells, CD20 is targeted with the antibody (Ab) retuximab (http://www.cancer.gov/cancertopics/druginfo/rituximab), which has been approved by the United States Food and Drug Administration (FDA) for use in monotherapy or in combination with a chemotherapeutic agent for the treatment of this disease (2). For enhanced efficacy, radionuclide-coupled anti-CD20 Abs tositumomab (http://us.gsk.com/products/assets/us_bexxar.pdf) (^131^I labeled) or ibritumomab (http://www.cancer.gov/drugdictionary/?CdrID=38483) (^90^Y conjugated) were also respectively approved by the FDA for the treatment of NHL and are commercially available in the United States. In addition, several anti-CD20 Abs, alone or in combination with different chemotherapeutic agents, are under evaluation for the treatment of various cancers in clinical trials (http://clinicaltrials.gov/ct2/results?term=anti+CD-20+antibodies&pg=1) approved by the FDA. In addition, Abs labeled with different nuclides have been used to detect and monitor cancers using imaging techniques such as positron emission tomography (PET) and single-photon emission computed tomography, but, due to long circulation and clearance times of the radiolabeled macromolecules (~150 kDa in size), investigators must wait for awhile before target/background ratios were reduced to suitable levels for imaging purposes (3, 4).

To circumvent the imaging problems encountered with intact radiolabeled Abs, two recombinant retuximab fragments, scFv-C_H_3 (a minibody; ~80 kDa in size) and a modified scFv-Fc fragment (~105 kDa in size), were generated, labeled with ^124^I, and evaluated by Olafsen et al. for in vivo imaging of human CD20-expressing lymphomas in mice (3). In this chapter, the biodistribution and imaging characteristics of the ^124^I-labeled minibody ([^124^I]-scFv-C_H_3) are described and compared with those of a ^64^Cu-labeled scFv-C_H_3 minibody ([^64^Cu]-scFv-C_H_3) used under the same experimental conditions. The biodistribution and imaging characteristics of the ^124^I-labeled scFv-Fc fragment ([^124^I]-scFv-Fc) are described and compared with those of [^124^I]-scFv-C_H_3 in a separate chapter of MICAD (www.micad.nih.gov) (5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+CD-20+minibody+production)]

The production, purification, and labeling of scFv-C_H_3 with ^124^I were done as described by Olafsen et al. (3). The efficiency of the minibody labeling reaction was reported to be 80.9% as determined with an instant thin-layer chromatography (ITLC) kit. The specific activity of [^124^I]-scFv-C_H_3 was reported to be 0.069 MBq/μg (1.86 μCi/μg). The stability and storage conditions used for [^124^I]-scFv-C_H_3 were not reported.

The minibody was also labeled with ^64^Cu as described by Olafsen et al. (3). The labeling efficiency of the reaction was reported to be 65.4% as determined with an ITLC kit. The specific activity of [^64^Cu]-scFv-C_H_3 was reported to be 0.042 MBq/μg (1.13 μCi/μg). The stability and storage conditions used for [^64^Cu]-scFv-C_H_3 were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti-cd20+minibody+in+vitro+studies)]

The binding of scFv-C_H_3 to CD20 was confirmed using an indirect immunofluorescence cell-surface staining method using 38C13-huCD20 cells (murine B cell lymphoma 38C13 cells transfected with and expressing the human CD20 gene) as detailed by Olafsen et al. (3) For this study, retuximab was used as a positive control. The immunoreactivity of [^124^I]-scFv-C_H_3 was determined by exposing an excess number of 38C13-huCD20 cells (exact cell number not reported) as described by Olafsen et al. (3). Immunoreactivity of the radiolabeled minibody was reported to be 37.7%. Although immunoreactivity of the radioiodinated minibody was low, the investigators showed that [^124^I]-scFv-C_H_3 could easily target CD20-expressing tumors under in vivo conditions (see below). The immunoreactivity of [^64^Cu]-scFv-C_H_3 was not reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti-cd20+minibody+rodentia)]

The biodistribution and tumor targeting of [^124^I]-scFv-C_H_3 were investigated in mice bearing either 38C13-huCD20 (expressing CD20) or 38C13 (not expressing CD20) cell tumors (n = 4 animals/cell type) (3). The animals were intravenously injected with the radiolabeled minibody and euthanized 4 h and 21 h later to study biodistribution of the tracer by retrieving the tumors and other major organs. Accumulated radioactivity in the different tissue types was presented as decay-corrected percent injected dose per gram tissue (% ID/g). The average uptake of radioactivity in the CD20-positive tumors at 21 h after the treatment was reported to be 12.9 ± 3.4% ID/g compared with the significantly lower (P = 0.003) accumulation of label in the CD20-nonexpressing tumors (1.9 ± 0.5% ID/g). Each of the major organs (liver, spleen, kidneys, and the lungs) were also reported to have a significantly lower (P = 0.05) uptake (<2.0% ID/g) compared with the CD20-positive tumors. The radioactivity uptake ratio of the CD20-positive/CD20-negative tumors was 7.0 ± 3.1, and the CD20-positive tumor/blood ratio was 4.7 ± 1.4 at 21 h after injection of the label. No blocking studies were reported.

Whole-body imaging of the animals was performed at 4 h and 21 h after injection of the radioiodinated minibody (3). An analysis of the images revealed that only the CD20-positive tumors had accumulated radioactivity 21 h after treatment with the labeled minibody. A region of interest (ROI) analysis of the images revealed that the CD20-positive/CD20-negative tumor ratios were 2.2 ± 0.8 at 4 h and 4.0 ± 0.7 at 21 h. In addition, the CD20-positive tumor/soft tissue ratio was observed to increase from 4.6 ± 0.4 at 4 h to 17.0 ± 6.7 at 21 h. No blocking studies were reported.

The biodistribution of [^64^Cu]-scFv-C_H_3 was also studied in mice bearing 38C13-huCD20 (n = 2 animals) or 38C13 (n = 3 animals) cell tumors for comparison with the biodistribution of [^124^I]-scFv-C_H_3 (3). The average uptake of radioactivity by the 38C13-huCD20 and 38C13 cell tumors with the ^64^Cu-labeled minibody at 19 h after the treatment was reported to be 6.5 ± 3.8% ID/g and 4.7 ± 1.7% ID/g, respectively, generating a ratio of 1.4 between the radioactivity accumulated in the 38C13-huCD20 and 38C13 cell tumors (the same ratio with the radioiodinated minibody was 7.0 at 21 h after the treatment). No blocking studies with [^64^Cu]scFv-C_H_3 were reported. An ROI analysis of images taken at 4 h and 19 h after treatment with the ^64^Cu-labeled minibody revealed that the CD20-positive/CD20-negative tumor ratios were 2.3 and 1.9, respectively, at these time points. These results suggested that, because of a high background, the use of [^64^Cu]-scFv-C_H_3 was less favorable than [^124^I]-scFv-C_H_3 for imaging purposes (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti-cd20+minibody+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## NIH Support

Studies reported in this chapter were supported by National Institutes of Health grants P50 CA107399, P50 CA086306, and CA119367 and a National Cancer Institute grant R24 CA86307.

## References

1 Cragg M.S., Walshe C.A., Ivanov A.O., Glennie M.J. (2005). The biology of CD20 and its potential as a target for mAb therapy. Curr Dir Autoimmun.
2 Bonavida B. (2007). Rituximab-induced inhibition of antiapoptotic cell survival pathways: implications in chemo/immunoresistance, rituximab unresponsiveness, prognostic and novel therapeutic interventions. Oncogene.
3 Olafsen T., Betting D., Kenanova V.E., Salazar F.B., Clarke P., Said J., Raubitschek A.A., Timmerman J.M., Wu A.M. (2009). Recombinant anti-CD20 antibody fragments for small-animal PET imaging of B-cell lymphomas. J Nucl Med.
4 Wu A.M., Olafsen T. (2008). Antibodies for molecular imaging of cancer. Cancer J.
5 Chopra, A., [124I] Labeled anti-CD20 modified scFv-Fc fragment [[124I]Anti-CD20 modified scFv-Fc fragment]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.